# [^18^F]-2-(2-Nitroimidazol-1H-yl)-(3,3,3-trifluoropropyl)acetamide

Chemical name: | [^18^F]-2-(2-Nitroimidazol-1H-yl)-N-(3,3,3-trifluoropropyl)acetamide
Abbreviated name: | [^18^F]EF3
Synonym:
Agent Category: | Compound
Target: | Hypoxic cells
Target Category: | Intracellular reduction and binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(18)F-EF3)]

In a variety of solid tumors, hypoxia was found to lead to tumor progression and the resistance of tumors to chemotherapy and radiotherapy (1-3). Tumor oxygenation is heterogeneously distributed within human tumors (4). Hypoxia in malignant tumors is thought to be a major factor limiting the efficacy of chemotherapy and radiotherapy. It would be beneficial to assess tumor oxygenation before and after therapy to provide an evaluation of tumor response to treatment and an insight into new therapeutic treatments (5). Tumor oxygenation is measured invasively using computerized polarographic oxygen-sensitive electrodes, which is regarded as the gold standard (6). Functional and non-invasive imaging of intra-tumoral hypoxia has been demonstrated to be feasible for the measurement of tumor oxygenation (7). This has led to the search and development of hypoxia-targeted, non-invasive markers of tumor hypoxia.

Chapman proposed the use of 2-nitroimidazoles for hypoxia imaging (8). 2-Nitroimidazole compounds are postulated to undergo reduction in hypoxic condition, forming highly reactive oxygen radicals that subsequently bind covalently to macromolecules inside the cells (9). [^18^F]Fluoromisonidazole ([^18^F]FMISO) is the most widely used positron emission tomography (PET) tracer for imaging tumor hypoxia (7). However, it has slow clearance kinetics and a high lipophilicity, resulting in substantially high background in PET scan. Novel 2-nitroimidazoles, such as [^18^F]FETA, [^18^F]FETNIM, 4-Br[^18^F]FPN, [^18^F]EF1, and [^18^F]EF5, are currently being investigated as potential markers of tumor hypoxia [PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=nitroimidazole+and+imaging)]. 2-(2-Nitroimidazol-1H-yl)-N-(3,3,3-trifluoropropyl)acetamide (EF3) is a 3-trifluorinated analog of EF1 (2-(2-nitro-1H-imidazol-1-yl)-N-(3-fluoropropyl)acetamide). EF3 binding to hypoxic tumor cells was shown to be dependent on oxygen and less dependent on the intracellular level of reductase system (10, 11). [^18^F]EF3 is being evaluated as a PET probe for detection of tumor hypoxia.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+EF3+synthesis)]

Josse et al. (12) reported that [^18^F]EF3 was synthesized by coupling 2,3,5,6-tetrafluorophenyl 2-(2-nitroimidazol-1-yl) acetate with [^18^F]-3,3,3-trifluoropropylamine in 5% radiochemical yield. [^18^F]-3,3,3-trifluoropropylamine was obtained with 40% overall chemical yield by oxidative [^18^F]-fluorodesulfurization of ethyl N-phthalimido-3-aminopropane dithioate, followed by deprotection with hydrazine. The total synthesis time was <90 min from the [^18^F]HF production in the cyclotron to the purification of [^18^F]EF3, which had a specific activity of 2.6 GBq/mmol (71 mCi/mmol) with a radiochemical purity >95%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+EF3+in+vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(18)F-EF3+rodentia)]

Mahy et al. (13) studied the biodistribution of [^18^F]EF3 in C3H mice bearing NFSA, FSA, FSA II, SCC VII, Sa-NH, or MCa-4 tumors under 10%, 21%, or 95% oxygen until the mice were euthanized 5–770 min after injection. The half-life in blood was 73.9 min. [^18^F]EF3 was eliminated mainly via the kidneys (75% of the injected activity was found in the urine by ~13 h). The biodistribution was fast and homogeneous except in the brain and bone, where it was significantly lower, and in the liver and the kidney, where it was significantly higher. In most organs, the exceptions being the gastrointestinal and urinary tracts, tissue/blood ratios were below or close to unity. There was a relative accumulation of the tracer in tumors with time (tumor/muscle ratios were 1.31–3.52, and tumor/blood ratios were 1.24–2.88 at 220 min after injection). In FSA II tumors, 10% oxygen (P = 0.004) significantly increased the tumor/muscle ratio, whereas 95% oxygen (P = 0.005) decreased it. [^18^F]EF3 was rapidly metabolized in the tumor, kidney, and liver with 49%, 6%, and 0.04% of the tracer intact at 30 min after injection, respectively. In other experiments, Mahy et al. (14) found a significant correlation (r^2^ = 0.57, P < 0.01) between the [^18^F]EF3 tumor/muscle ratio and the fluorescence intensity of EF5 in the mice bearing tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+EF3+(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+EF3+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+EF3+human)]

No publication is currently available.

.

## References

1 Serkies K., Jassem J. (2005). Chemotherapy in the primary treatment of cervical carcinoma. Crit Rev Oncol Hematol.
2 Vaupel P., Mayer A. (2005). Hypoxia and anemia: effects on tumor biology and treatment resistance. Transfus Clin Biol.
3 Rajendran J.G., Krohn K.A. (2005). Imaging hypoxia and angiogenesis in tumors. Radiol Clin North Am.
4 Vaupel P., Harrison L. (2004). Tumor hypoxia: causative factors, compensatory mechanisms, and cellular response. Oncologist.
5 Dehdashti F., Grigsby P.W., Mintun M.A., Lewis J.S., Siegel B.A., Welch M.J. (2003). Assessing tumor hypoxia in cervical cancer by positron emission tomography with 60Cu-ATSM: relationship to therapeutic response-a preliminary report. Int J Radiat Oncol Biol Phys.
6 Raleigh J.A., Dewhirst M.W., Thrall D.E. (1996). Measuring Tumor Hypoxia. Semin Radiat Oncol.
7 Foo S.S., Abbott D.F., Lawrentschuk N., Scott A.M. (2004). Functional imaging of intratumoral hypoxia. Mol Imaging Biol.
8 Chapman J.D. (1979). Hypoxic sensitizers--implications for radiation therapy. N Engl J Med.
9 Chapman J.D., Baer K., Lee J. (1983). Characteristics of the metabolism-induced binding of misonidazole to hypoxic mammalian cells. Cancer Res.
10 Cobb L.M., Nolan J., Hacker T. (1992). Retention of misonidazole in normal and malignant tissues: interplay of hypoxia and reductases. Int J Radiat Oncol Biol Phys.
11 Franko A.J., Koch C.J., Garrecht B.M., Sharplin J., Hughes D. (1987). Oxygen dependence of binding of misonidazole to rodent and human tumors in vitro. Cancer Res.
12 Josse O., Labar D., Georges B., Gregoire V., Marchand-Brynaert J. (2001). Synthesis of [18F]-labeled EF3 [2-(2-nitroimidazol-1-yl)-N-(3,3,3-trifluoropropyl)-acetamide], a marker for PET detection of hypoxia. Bioorg Med Chem.
13 Mahy P., De Bast M., Leveque P.H., Gillart J., Labar D., Marchand J., Gregoire V. (2004). Preclinical validation of the hypoxia tracer 2-(2-nitroimidazol-1-yl)- N-(3,3,3-[(18)F]trifluoropropyl)acetamide, [(18)F]EF3. Eur J Nucl Med Mol Imaging.
14 Mahy P., De Bast M., Gillart J., Labar D., Gregoire V. (2006). Detection of tumour hypoxia: comparison between EF5 adducts and [18F]EF3 uptake on an individual mouse tumour basis. Eur J Nucl Med Mol Imaging.